# Anti-vascular cell adhesion molecule-1 monoclonal antibody M/K-2.7 microbubbles

Chemical name: | Anti-vascular cell adhesion molecule-1 monoclonal antibody M/K-2.7 microbubbles
Abbreviated name: | MB_VCAM-1_
Synonym:
Agent category: | Antibody
Target: | Vascular cell adhesion molecule-1 (VCAM-1)
Target category: | Adhesion molecule
Method of detection: | Ultrasound (US)
Source of signal: | Microbubbles
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=54648638), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=46249772) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412) for more information about VCAM-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+microbubble)]

Ultrasound is widely used imaging modality (1), and its role in noninvasive molecular imaging with ligand-carrying microbubbles (MBs) is expanding (2). MBs are spherical cavities encapsulated in a shell and filled by a gas. The shells are made of phospholipids, surfactants, denatured human serum albumin, or synthetic polymers. Ligands and antibodies can be incorporated into the MB shell surface. MBs are usually 2–8 μm in diameter. MBs of this size provide a strongly reflective interface and resonate to ultrasound waves. They are used as ultrasound contrast agents in imaging of inflammation, angiogenesis, intravascular thrombus, and tumors (2-4). They also can potentially be used for drug and gene delivery (5).

Endothelial cells are important cells in inflammatory responses (6, 7). Bacterial lipopolysaccharide (LPS), virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokine and chemokine secretion. Leukocyte emigration from blood is dependent on their ability to roll along and subsequently adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell surface adhesion molecules, such as intracellular adhesion molecule-1 (ICAM-1), vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic toward leukocytes and toward sites of inflammation and tissue injury. The movements of leukocytes through endothelial junctions into the extravascular space are highly orchestrated through various interactions with different adhesion molecules on endothelial cells (8).

VCAM-1 is found in very low amounts on the cell surface of resting endothelial cells and other vascular cells, such as smooth muscle cells and fibroblasts (9-13). VCAM-1 binds to its counterligand very late antigen-4 (VLA-4) integrin on the cell-surface of leukocytes. IL-1 and TNFα increase expression of VCAM-1 and other cell adhesion molecules on the vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. Furthermore, VCAM-1 expression was also induced by oxidized low-density lipoproteins under atherogenic conditions (14). Overexpression of VCAM-1 by atherosclerotic lesions plays an important role in their progression towards vulnerable plaques, which may erode and rupture. MBs targeted with antibodies against VCAM-1 are being developed as a noninvasive agent for VCAM-1 expression in vascular endothelial cells during different stages of inflammation in atherosclerosis (15).

### Related Resource Links:

- Chapters in MICAD (VCAM-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=VCAM-1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (VCAM-1 (http://www.ncbi.nlm.nih.gov/gene/7412))
- Articles in Online Mendelian Inheritance in Man (OMIM) (VCAM-1 (http://www.ncbi.nlm.nih.gov/omim/192225))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+attachment)]

For targeted MBs, Kaufmann et al. (15) prepared biotinylated MBs by sonication of an aqueous dispersion of decafluorobutane gas, distearoylphosphatidylcholine, polyoxyethylene-40-stearate, and distearoylphosphatidylethanolamine-polyethyleneglycol-biotin. MBs were combined with streptavidin, washed, and conjugated with biotinylated mouse monoclonal antibody M/K-2.7 against VCAM-1 (MB_VCAM-1_) or isotype control monoclonal antibody (MB_c_). The MBs were about 3-4 μm in diameter. An antibody/MB ratio was estimated to be >50,000 by flow cytometry.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+in+vitro)]

Kaufmann et al. (15) reported that MB_VCAM-1_ (3 × 10^6^/ml) perfused through the flow chamber coated with endothelial cells at a wall-shear rate of 0.5-12.0 dynes/cm^2^. There was a significantly greater number of MB_VCAM-1_ attached to TNF^_^activated endothelial cells than to normal endothelial cells at 0.5 dynes/cm^2^ (P <0.05). The number of MB_VCAM-1_ adherent to activated endothelial cells decreased with increasing shear rate. No attachment of MBc to normal and activated endothelial cells was observed.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+rodentia)]

Kaufmann et al. (15) studied MB_VCAM-1_ attachment to aortic plaque by microscopy of the thoracic aorta 10 min after intravenous injection in wild-type or apolipoprotein E–deficient (apoE^-/-^) mice on either normal chow or hypercholesterolemic diet. Contrast-enhanced ultrasound (CEU) molecular imaging of the thoracic aorta 10 min after intravenous MB injection was performed for the same animal groups. Aortic attachment of MB_VCAM-1_ and CEU signal were very low in control wild-type mice on normal chow diet, whereas apoE^-/-^ mice on hypercholesterolemic diet exhibited the highest attachment and signal. Aortic attachment of MB_VCAM-1_ and CEU signal for MB_VCAM-1_ differed between treatment groups according to the extent of VCAM-1–positive plaque formation (median CEU videointensity was 1.8, 3.7, 6.8, and 11.2 for wild-type mice on normal chow diet, wild-type mice on hypercholesterolemic diet, apoE^-/-^ mice on normal chow diet, and apoE^-/-^ mice on hypercholesterolemic diet, respectively; P < 0.001). On the other hand, MB_c_ exhibited minimal contrast in all groups.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+human)]

No publication is currently available.

## NIH support

R01 DK063508, R01 HL074443, R01 HL078610

## References

1 Wells P.N. (2001). Physics and engineering: milestones in medicine. Med Eng Phys.
2 Lindner J.R. (2004). Microbubbles in medical imaging: current applications and future directions. Nat Rev Drug Discov.
3 Klibanov A.L. (2005). Ligand-carrying gas-filled microbubbles: ultrasound contrast agents for targeted molecular imaging. Bioconjug Chem.
4 Villanueva F.S., Wagner W.R., Vannan M.A., Narula J. (2004). Targeted ultrasound imaging using microbubbles. Cardiol Clin.
5 Dijkmans P.A., Juffermans L.J., Musters R.J., van Wamel A., ten Cate F.J., van Gilst W., Visser C.A., de Jong N., Kamp O. (2004). Microbubbles and ultrasound: from diagnosis to therapy. Eur J Echocardiogr.
6 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
7 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
8 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
9 Bochner B.S., Luscinskas F.W., Gimbrone M.A., Newman W., Sterbinsky S.A., Derse-Anthony C.P., Klunk D., Schleimer R.P. (1991). Adhesion of human basophils, eosinophils, and neutrophils to interleukin 1-activated human vascular endothelial cells: contributions of endothelial cell adhesion molecules. J Exp Med.
10 Kume N., Cybulsky M.I., Gimbrone M.A. (1992). Lysophosphatidylcholine, a component of atherogenic lipoproteins, induces mononuclear leukocyte adhesion molecules in cultured human and rabbit arterial endothelial cells. J Clin Invest.
11 Leung K.H. (1999). Release of soluble ICAM-1 from human lung fibroblasts, aortic smooth muscle cells, dermal microvascular endothelial cells, bronchial epithelial cells, and keratinocytes. Biochem Biophys Res Commun.
12 Luscinskas F.W., Cybulsky M.I., Kiely J.M., Peckins C.S., Davis V.M., Gimbrone M.A. (1991). Cytokine-activated human endothelial monolayers support enhanced neutrophil transmigration via a mechanism involving both endothelial-leukocyte adhesion molecule-1 and intercellular adhesion molecule-1. J Immunol.
13 Nagel T., Resnick N., Atkinson W.J., Dewey C.F., Gimbrone M.A. (1994). Shear stress selectively upregulates intercellular adhesion molecule-1 expression in cultured human vascular endothelial cells. J Clin Invest.
14 Aikawa M., Libby P. (2004). The vulnerable atherosclerotic plaque: pathogenesis and therapeutic approach. Cardiovasc Pathol.
15 Kaufmann B.A., Sanders J.M., Davis C., Xie A., Aldred P., Sarembock I.J., Lindner J.R. (2007). Molecular imaging of inflammation in atherosclerosis with targeted ultrasound detection of vascular cell adhesion molecule-1. Circulation.